# Indocyanine green derivative 02-Glu-c(RGDyK)_2_

Chemical name: | Indocyanine green derivative 02-Glu-c(RGDyK)_2_
Abbreviated name: | ICG-Der-02-c(RGDyK)_2_
Synonym: | c(RGDyK)_2_-ICG-Der-02
Agent category: | Peptide
Target: | α_v_β_3_ integrin
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal/contrast: | ICG-Der-02
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive complement to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (5-8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (9). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (10-17). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (12, 16, 18). Various radiolabeled (such as ^18^F, ^64^Cu, ^68^Ga, and ^99m^Tc) and NIR fluorescence-labeled (such as Cy5.5, Cy7, and Cypate) RGD peptides have been introduced for imaging of tumors and tumor angiogenesis (19). ICG derivative 02 (ICG-Der-02), a hydrophilic dye, contains one carboxyl functional group for covalent conjugation to the amino group of biomolecules. Cao et al. (20) conjugated ICG-Der-02 via the α-amino group of Glu residue of Glu-c(RGDyK)_2_ (dimer) peptide to form ICG-Der-02-c(RGDyK)_2._ ICG-Der-02 was also conjugated to the Ɛ-amino group of the lysine residue of RGD (linear) and c(RGDyK) (monomer) to form ICG-Der-02-RGD and ICG-Der-02-c(RGDyK), respectively. The three ICD-Der-02-labeled conjugates were evaluated for in vivo NIR optical imaging in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8), RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02)]

ICG-Der-02-N-hydroxysuccinimide ester (0.01 mmol) was reacted with RGD (linear), c(RGDyK), or Glu-c(RGDyK)_2_ (0.01 mmol) in sodium borate buffer (pH 8.3) for 18 h at room temperature (20). The ICG-Der-02 conjugates were purified with high-performance liquid chromatography and verified with mass spectroscopy. There is one dye molecule per conjugate. The yields and purities of ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_ were not reported. ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_ displayed spectral properties similar to those of ICG-Der-02 (maximum absorption at 783 nm and maximum emission at 830–834 nm), with quantum yields of 13.6%, 14.3%, and 13.9%, respectively. The quantum yield of ICG-Der-02 was 13.0%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02%20and%20in%20vitro)]

In vitro photostability studies of ICG-Der-02, ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_ showed that the three ICG-Der-02 conjugates (22.7%–26.1% reduction) exhibited higher photostability than ICG-Der-02 (45.4%–46.8% reduction) in borate buffer and human plasma after 60 min of irradiation at 765.9 nm (20). Rhodamine (RhB)-labeled RGD probes showed high fluorescence signals in α_v_β_3_-expressing MDA-MB-231 human breast cancer and U87MG human glioblastoma with intensity order dimer > monomer > linear. On the other hand, α_v_β_3_-negative MCF-7 human breast tumor cells exhibited much weaker fluorescence than MDA-MB-231 and U87MG cells with the three RGD-based probes. Laser confocal microscopy showed binding of RGD-based probes in the cell surface and cytoplasm of the cells. Excess non-conjugated RGD peptides blocked the fluorescence signals. RhB was used because the investigators do not have confocal fluorescence microcopy with NIR capability.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02%20and%20rodentia)]

Cao et al. (20) performed in vivo whole-body NIR fluorescence imaging studies in normal nude mice (n = 5) at 0–24 h after intravenous injection of 2 nmol ICG-Der-02, ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), or ICG-Der-02-c(RGDyK)_2_. Images showed that NIR fluorescence spread over the body at 1 h and then concentrated in the kidneys and urinary bladder. Most NIR fluorescence was cleared from the body by 24 h. The kidney/muscle ratios peaked at 4 h, with 9–10 for the RGD-based probes and 8 for the dye alone. The liver/muscle ratios peaked at 1 h, with ~3 for the dye and RGD-based probes. Ex vivo imaging of the main organs (the liver, kidneys, lung, intestine, heart, and spleen) of mice was performed at 6 h. NIR fluorescence was detected mainly in the kidneys, whereas little NIR fluorescence was observed in the other organs. Blood NIR fluorescence levels of the dye and RGD-based probes peaked at 1 h and then gradually declined to background by 6 h. No obvious differences were observed in the biodistribution of the dye and RGD-based probes, which were mainly excreted by the kidneys.

Cao et al. (20) performed in vivo whole-body NIR fluorescence imaging studies in nude mice (n = 5/group) bearing MDA-MB-231, U87MG, or MCF-7 xenografts at 0, 1, 4, 6, 12, 24, and 48 h after injection of 2 nmol ICG-Der-02, ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), or ICG-Der-02-c(RGDyK)_2_. For the MDA-MB-231 tumors, all three probes and ICG-Der-02 identified the tumors, with maximum fluorescence intensity at 4 h, and then cleared through the renal pathway. The tumor/muscle ratios at 4 h were 3.0, 3.6, 5.5, and 6.8 for ICG-Der-02, ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_, respectively. At 48 h, the tumor/muscle ratios were 1.2, 2.3, 3.0, and 3.5, respectively. Blocking experiments were performed with co-injection of excess corresponding non-conjugated RGD peptides with 63%, 70%, and 75% reduction of fluorescence intensity in the tumor for ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_, respectively. Ex vivo imaging at 4 h showed the tumor/background ratios were 10, 17, 28, and 34 for ICG-Der-02, ICG-Der-02-RGD, ICG-Der-02-c(RGDyK), and ICG-Der-02-c(RGDyK)_2_, respectively. The organ with the highest tissue/background ratio was the kidney (~22), followed by the liver (~7), lung (~7), intestine (~6), spleen (~3), and heart (~3). No obvious differences were observed in the normal organs amongst the dye and probes. For the U87MG tumor, whole-body NIR fluorescence imaging scans showed slightly weaker NIR fluorescence signals (dimer > monomer > linear RGD peptides) than the MDA-MD-231 tumor, whereas minimal NIR fluorescence signals were observed in the α_v_β_3_-negative MCF-7 tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD+ICG-Der-02%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
6 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
7 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
8 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
9 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
10 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
11 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Varner J.A., Cheresh D.A. (1996). Integrins and cancer. Curr Opin Cell Biol.
15 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
16 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
17 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
18 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
19 Haubner R., Beer A.J., Wang H., Chen X. (2010). Positron emission tomography tracers for imaging angiogenesis. Eur J Nucl Med Mol Imaging.
20 Cao J., Wan S., Tian J., Li S., Deng D., Qian Z., Gu Y. (2012). Fast clearing RGD-based near-infrared fluorescent probes for in vivo tumor diagnosis. Contrast Media Mol Imaging.